# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-p-benzyl-NH-hu14.18K322A

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-p-benzyl-NH-hu14.18K322A
Abbreviated name: | ^64^Cu-DOTA-Bn-NH-hu14.18K322A, ^64^Cu-p-NH_2_-Bn-DOTA-hu14.18K322A
Synonym:
Agent category: | Antibody
Target: | Disialoganglioside GD2
Target category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hu14.18)]

Disialoganglioside GD2 is a glycolipid on cell surfaces of neurons that involves cell–matrix interactions (1). GD2 is highly expressed on tumors of neuroectodermal origin, such as neuroblastoma and melanoma cells, whereas GD2 is weakly expressed on most normal cells (2). Therefore, GD2 is a useful target for both identification and treatment of tumor cells with monoclonal antibodies (mAbs), such as chimeric mAb ch14.18 and humanized mAb hu14.18 (3, 4). Both mAbs are now in clinical trials (http://www.clinicaltrials.gov/ct2/results?term=14.18&Search=Search) for treatment of melanoma and neuroblastoma. hu14.18K322A, a variant of hu14.18 with a single-spot mutation, was developed to decrease complement activation to minimize cytotoxic side effects of ch14.18 and hu14.18 (5). Vavere et al. (6) evaluated ^64^Cu-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-p-benzyl-NH-hu14.18K322A (^64^Cu-DOTA-Bn-NH-hu14.18K322A) for use with positron emission tomography (PET) imaging of GD2 expression in nude mice bearing human tumors.

### Related Resource Links:

- Chapters in MICAD (disialoganglioside (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=(GD2%20OR%20disialoganglioside)+AND+micad%5Bbook%5D))
- Clinical trials (ch14.18 (http://www.clinicaltrials.gov/ct2/results?term=ch14.18), hu14.18 (http://www.clinicaltrials.gov/ct2/results?term=hu14.18), hu14.18K322A (http://www.clinicaltrials.gov/ct2/results?term=hu14.18K322A&Search=Search))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hu14.18+synthesis)]

The DOTA-Bn-NH_2_ chelator was conjugated through its primary aromatic amine group to the carboxyl groups of the glutamate and aspartate residues of the hu14.18K322A mAb at a 500:1 ratio in the presence of 1-ethyl-3-(3-dimethylaminopropyl)-carbodiimide (EDC) (6). EDC was added to the mAb in a ratio of 250:1 in 0.1 M sodium acetate buffer (pH = 5.0) and incubated for 30 min at 37°C. DOTA-Bn-NH-hu14.18K322A was purified with high-performance liquid chromatography (HPLC). DOTA-Bn-NH-hu14.18K322A was radiolabeled using ^64^CuCl_2_ in sodium acetate buffer (pH 5.0) for 30 min at 37°C. The radiochemical purity was >95%, as determined with HPLC. Specific activities of ^64^Cu-DOTA-Bn-NH-hu14.18K322A were reported to be 19–56 MBq/nmol (0.5–1.5 mCi/nmol). There were 2.5–4.7 DOTA moieties per mAb as determined with serial isotope dilution experiments.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hu14.18+in+vitro)]

^64^Cu-DOTA-Bn-NH-hu14.18K322A had immunoreactivity similar to that of unconjugated mAb as determined with binding to purified GD2 (6). hu14.18K322A inhibited the binding of ^64^Cu-DOTA-Bn-NH-hu14.18K322A to GD2 (IC_50_ value, 14 nM). Cellular accumulation of ^64^Cu-DOTA-Bn-NH-hu14.18K322A was performed in culture with M21 human melanoma (GD2-positive) and PC-3 human prostate adenocarcinoma (GD2-negative) cells for 60 min at 37°C. Radioactivity increased from 0.13%/mg protein at 5 min to 0.46%/mg at 60 min in the M21 cells, whereas radioactivity in the PC-3 cells was 0.07%/mg at 60 min. Co-incubation with 360-fold excess hu14.18K322A inhibited the radioactivity levels at 60 min in the M21 and PC-3 cells by 80% and 20%, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hu14.18+%20rodentia)]

Vavere et al. (6) performed ex vivo biodistribution studies in nude mice (n = 4–6/group) bearing M21 or PC-3 xenografts at 24 h after injection of 1.82–2.41 MBq (50–65 µCi) ^64^Cu-DOTA-Bn-NH-hu14.18K322A. The radioactivity levels in all organs were higher in the mice bearing M21 tumors than in those with PC-3 tumors. The radioactivity levels in the M21 and PC-3 tumors were 9.52 ± 2.55% injected dose/gram (ID/g) and 4.96 ± 0.51% ID/g (P < 0.0023), respectively. The radioactivity levels in the blood in the M21- and PC-3-bearing mice were 14.8 ± 1.3% ID/g and 11.4 ± 0.5% ID/g (P < 0.0003), respectively. The organ with the highest radioactivity levels (M21 tumors versus PC-3 tumors) was the lung (9.93% ID/g versus 7.26% ID/g), followed by the liver (7.14% ID/g versus 5.58% ID/g), spleen (6.79% ID/g versus 4.55% ID/g), kidney (5.10% ID/g versus 4.59% ID/g), heart (4.36% ID/g versus 3.27% ID/g), and bone (2.37% ID/g versus 1.79% ID/g). The investigators suggested that the high background accumulation in the PC-3 tumors may be due to the enhanced permeability and retention effect. However, no blocking studies were performed.

PET scans were performed after intravenous injection of 5.2 MBq (140 μCi) ^64^Cu-DOTA-Bn-NH-hu14.18K322A in six nude mice bearing M21 and PC-3 tumors at 1, 24, and 48 h after injection (6). High accumulation of the label was evident in the GD2-positive M21 tumors, with low accumulation the GD2-negative PC-3 tumors, at 24 h and 48 h. The radioactivity level in the M21 tumors increased from 4.75% ID/cm^3^ at 24 h to 6.45% ID/cm^3^ at 48 h, whereas the radioactivity levels in the PC-3 tumors were 3.78% ID/cm^3^ and 3.67% ID/cm^3^ at 24 h and 48 h, respectively. PET images showed that the radioactivity distribution pattern was similar with the ex vivo biodistribution data. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hu14.18+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hu14.18+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hu14.18+human)]

No publication is currently available.

## NIH Support

R24 CA86307

## References

1 Rabu C., McIntosh R., Jurasova Z., Durrant L. (2012). Glycans as targets for therapeutic antitumor antibodies. Future Oncol.
2 Modak S., Cheung N.K. (2007). Disialoganglioside directed immunotherapy of neuroblastoma. Cancer Invest.
3 Mueller B.M., Reisfeld R.A., Gillies S.D. (1990). Serum half-life and tumor localization of a chimeric antibody deleted of the CH2 domain and directed against the disialoganglioside GD2. Proc Natl Acad Sci U S A.
4 Mueller B.M., Romerdahl C.A., Gillies S.D., Reisfeld R.A. (1990). Enhancement of antibody-dependent cytotoxicity with a chimeric anti-GD2 antibody. J Immunol.
5 Sorkin L.S., Otto M., Baldwin W.M., Vail E., Gillies S.D., Handgretinger R., Barfield R.C. (2010). H. Ming Yu, and A.L. Yu, Anti-GD(2) with an FC point mutation reduces complement fixation and decreases antibody-induced allodynia. Pain.
6 Vavere A.L., Butch E.R., Dearling J.L., Packard A.B., Navid F., Shulkin B.L., Barfield R.C., Snyder S.E. (2012). 64Cu-p-NH2-Bn-DOTA-hu14.18K322A, a PET Radiotracer Targeting Neuroblastoma and Melanoma. J Nucl Med.